# 1-Deoxy-1-[^18^F]fluoro-scyllo-inositol

Chemical name: | 1-Deoxy-1-[^18^F]fluoro-scyllo-inositol
Abbreviated name: | [^18^F]-scyllo-Inositol
Synonym:
Agent category: | Compound
Target: | Na+-dependent myo-inositol cotransporter
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20sycllo-Inositol)]

Inositol exists in nine possible stereoisomers, of which myo-inositol and scyllo-inositol are widely present (1). Inositol is a substrate for kinases to form a number of secondary messengers in cells, such as inositol phosphates, phosphatidylinositol, and phosphatidylinositol phosphate (2). scyllo-Inositol has been shown to interact with β-amyloid (Aβ_1-42_) peptides (3, 4), and phosphatidylinositol inhibits fibrillogenesis (5). scyllo-Inositol is currently in clinical trials for the treatment of Alzheimer’s disease. myo-Inositol and scyllo-inositol are actively transported into cells primarily by the Na+-dependent myo-inositol cotransporter system (1). scyllo-Inositol has been detected in human breast tumor extracts and may serve as a marker for breast cancer (6). In comparison with 2-[^18^F]fluoro-2-deoxy-D-glucose ([^18^F]FDG), 1-deoxy-1-[^18^F]fluoro-scyllo-inositol ([^18^F]-scyllo-inositol) has been evaluated as a positron emission tomography (PET) tracer for imaging of inflammation as well as breast and brain cancer xenografts in nude mice (7, 8).

### Related Resource Links:

- Chapters in MICAD (myo-Inositol cotransporter (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=myo-Inositol%20cotransporter+AND+micad%5Bbook%5D))
- Gene information in NCBI (myo-Inositol cotransporter (http://www.ncbi.nlm.nih.gov/gene/6526))
- Articles in Online Mendelian Inheritance in Man (OMIM) (myo-Inositol cotransporter (http://omim.org/entry/600444))
- Clinical trials (myo-Inositol (http://www.clinicaltrials.gov/ct2/results?term=myo-inositol))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20scyllo-inositol%20and%20synthesis)]

Vasdev et al. (8) reported the synthesis of [^18^F]-scyllo-inositol in an one-pot, three-step reaction. 1,6:3,4-Bis-[O-(2,3-dimethyoxybutane-2,3-diyl)]-2-O-trifluoromethanesulfonyl-5-O-benzoyl-myo-inositol was fluorinated in the presence of K[^18^F]F/K2.2.2/K_2_CO_3_ (90°C, 15 min), followed by trifluoroacetic acid hydrolysis of the diacetals (90°C, 15 min) and sodium hydroxide hydrolysis of the benzoyl group (90°C, 15 min). [^18^F]-scyllo-Inositol was purified with column chromatography. The total radiosynthesis time was 80 min, with a radiochemical yield of 16 ± 3% (n = 6) and a radiochemical purity of >98% at the end of synthesis (EOS). The specific activity of [^18^F]-scyllo-inositol was not reported. McLarty et al. (7) prepared [^18^F]-scyllo-inositol using a radiosynthesis module with a radiochemical yield of 24.6 ± 3.3% (n = 5) and a radiochemical purity of >99% at EOS. The total synthesis time was ~65 min, with specific activities of 880 ± 550 GBq/µmol (23.8 ± 14.9 Ci/µmol) at EOS. The logD of [^18^F]-scyllo-inositol was measured to be −2.8 ± 0.3.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20scyllo-inositol%20acid%20and%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20scyllo-inositol%20acid%20and%20rodentia)]

McLarty et al. (7) performed ex vivo biodistribution studies in female nude mice (n = 3–5/group) bearing MDA-MB-361, MCF-7, and MDA-MB-231 human breast cancer cells and turpentine-induced inflammation after intravenous injection of [^18^F]-scyllo-inositol or [^18^F]FDG at 60 min. The organs with the highest and lowest accumulation of [^18^F]-scyllo-inositol were the kidney (~40% injected dose/gram (ID/g)) and brain (~0.5% ID/g), respectively. In contrast, the organs with highest accumulation of [^18^F]FDG were the heart (~37% ID/g) and brain (~9% ID/g). There was no significant difference in the accumulation of [^18^F]FDG among the three breast tumors (5.4%–5.9% ID/g). The accumulation of [^18^F]-scyllo-inositol in the three breast tumors (3.2%–4.6% ID/g) was slightly lower than that of [^18^F]FDG. The tumor/blood ratios of [^18^F]-scyllo-inositol in MDA-MB-361, MCF-7, and MDA-MB-231 tumors (1.2–1.5) were lower than those of [^18^F]FDG (4.7–8.1) (P < 0.05). On the other hand, the tumor/muscle ratios of [^18^F]-scyllo-inositol in the three tumors (2.8–4.0) were higher than those of [^18^F]FDG (1.6–1.9) (P < 0.05). The tumor/inflammation ratio of [^18^F]-scyllo-inositol (1.4 ± 0.2) was slightly higher than that of [^18^F]FDG (1.0 ± 0.3).

PET imaging studies were performed with 7.6 MBq (0.21 mCi) [^18^F]-scyllo-inositol or [^18^F]FDG at 60 min after injection in female nude mice (n = 3–5/group) with the three tumors and turpentine-induced inflammation, which were clearly visualized. Volume of interest (VOI) analysis of radioactivity accumulation in the three tumors and inflammation was consistent with the ex vivo biodistribution studies. No blocking studies were performed.

In another experiment, nude mice were implanted intracranially with U-87 MG human glioma tumors (7). The accumulation levels of [^18^F]-scyllo-inositol in the tumors and brain were 4.4 ± 0.6% ID/g and 0.4 ± 0.1% ID/g, respectively. In contrast, the accumulation levels of [^18^F]FDG in the tumors and brain were 22.6 ± 5.8% ID/g and 11.0 ± 1.5% ID/g, respectively. The tumor/blood ratio of [^18^F]-scyllo-inositol (1.3 ± 0.3) was significantly lower than that of [^18^F]FDG (17.8 ± 8.1) (P < 0.05), whereas the tumor/brain ratio of [^18^F]-scyllo-inositol (10.6 ± 2.5) was significantly higher than that of [^18^F]FDG (2.1 ± 0.6) (P < 0.01). PET imaging with VOI analysis showed that the tumor accumulation of [^18^F]FDG (20.1 ± 5.2) was higher than that of [^18^F]-scyllo-inositol (5.5 ± 0.5) (P < 0.01). On the other hand, the normal brain accumulation of [^18^F]-scyllo-inositol (1.1 ± 0.2) was significantly lower than that of [^18^F]FDG (11.7 ± 2.6) (P < 0.01). The tumor/brain ratios were 5.0 and 1.7 (P < 0.01) for [^18^F]-scyllo-inositol and [^18^F]FDG, respectively. No blocking studies were performed. The accumulation of [^18^F]-scyllo-Inositol in the tumors as inositol phosphates, phosphatidylinositol, and phosphatidylinositol phosphate was not demonstrated.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20scyllo-inositol%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20scyllo-inositol%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20scyllo-inositol%20and%20human)]

No publication is currently available.

## References

1 Fisher S.K., Novak J.E., Agranoff B.W. (2002). Inositol and higher inositol phosphates in neural tissues: homeostasis, metabolism and functional significance. J Neurochem.
2 Seeds A.M., York J.D. (2007). Inositol polyphosphate kinases: regulators of nuclear function. Biochem Soc Symp.
3 Sun Y., Zhang G., Hawkes C.A., Shaw J.E., McLaurin J., Nitz M. (2008). Synthesis of scyllo-inositol derivatives and their effects on amyloid beta peptide aggregation. Bioorg Med Chem.
4 Hawkes C.A., Deng L.H., Shaw J.E., Nitz M., McLaurin J. (2010). Small molecule beta-amyloid inhibitors that stabilize protofibrillar structures in vitro improve cognition and pathology in a mouse model of Alzheimer's disease. Eur J Neurosci.
5 Dasilva K.A., Shaw J.E., McLaurin J. (2010). Amyloid-beta fibrillogenesis: structural insight and therapeutic intervention. Exp Neurol.
6 Gribbestad I.S., Fjosne H.E., Haugen O.A., Nilsen G., Krane J., Petersen S.B., Kvinnsland S. (1993). In vitro proton NMR spectroscopy of extracts from human breast tumours and non-involved breast tissue. Anticancer Res.
7 McLarty K., Moran M.D., Scollard D.A., Chan C., Sabha N., Mukherjee J., Guha A., McLaurin J., Nitz M., Houle S., Wilson A.A., Reilly R.M., Vasdev N. (2011). Comparisons of [18F]-1-deoxy-1-fluoro-scyllo-inositol with [18F]-FDG for PET imaging of inflammation, breast and brain cancer xenografts in athymic mice. Nucl Med Biol.
8 Vasdev N., Chio J., van Oosten E.M., Nitz M., McLaurin J., Vines D.C., Houle S., Reilly R.M., Wilson A.A. (2009). Synthesis and preliminary biological evaluations of [18F]-1-deoxy-1-fluoro-scyllo-inositol. Chem Commun (Camb).